# ^64^Cu-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-TNYLFSPNGPIARAW (TNYL-RAW)

Chemical name: | ^64^Cu-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid- TNYLFSPNGPIARAW (TNYL-RAW)
Abbreviated name: | ^64^Cu-DOTA-TNYL-RAW
Synonym:
Agent category: | Peptide
Target: | Ephrin receptor B4 (EphB4)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TNYL-RAW)]

The ephrin (Eph) receptors constitute the largest member of the receptor tyrosine kinase family (1, 2). The Eph receptors and their ligands (ephrins) mediate numerous biological processes in normal development, particularly in the nervous and cardiovascular systems (3-5). Based on their structures and sequence relationships, ephrins are divided into the ephrin-A class, which are anchored to the cell membrane by a glycosylphosphatidylinositol linkage, and the ephrin-B class, which are transmembrane proteins. The Eph family of receptors is divided into two groups, EphA and EphB, on the basis of the similarity of their extracellular domain sequences and their affinities for binding ephrin-A and ephrin-B ligands. The Eph receptors transmit forward signals via their kinase domain and reverse signals via their transmembrane ephrin ligands (6). EphB–ephrin-B interactions are capable of mediating bi-directional signaling events upon cell–cell contact, either into the receptor-expressing cell as "forward signaling" or into the ligand-expressing cell as "reverse signaling" (7).

Ephrin-2 is expressed on arterial and activated endothelial cells, whereas EphB4 is normally expressed on venous endothelial cells and various blood cells (8). EphB4 selectively binds to ephrin-2 to promote cell signaling and angiogenesis. EphB4 has been implicated in cancer progression and in pathological forms of angiogenesis. Overexpression of EphB4 has been observed in cancer cells and is associated with tumorigenesis via forward signaling and angiogenesis via reverse signaling through ephrin-2 interaction (9). EphB4 forward signaling stimulates cellular proliferation. Koolpe et al. (10) identified a 15-mer peptide, Tyr-Asn-Tyr-Leu-Phe-Ser-Pro-Asn-Gly-Pro-Ile-Ala-Arg-Ala-Trp (TNYL-RAW), to be a selective antagonist of EphB4 using phage display screening. Xiong et al. (11) reported the development of ^64^Cu-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-TNYL-RAW (^64^Cu-DOTA-TNYL-RAW) for positron emission tomography (PET) imaging of EphB4 in nude mice bearing tumor xenografts.

### Related Resource Links:

- Chapters in MICAD (EphB4 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=EphB4+AND+micad%5Bbook%5D))
- Gene information in NCBI (EphB4 (http://www.ncbi.nlm.nih.gov/gene?term=2050), ephrin-B2 (http://www.ncbi.nlm.nih.gov/gene/1948))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EphB4 (http://www.ncbi.nlm.nih.gov/omim/600011), ephrin-B2 (http://www.ncbi.nlm.nih.gov/omim/600527))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TNYL-RAW+synthesis)]

TNYL-RAW peptide was prepared using solid-phase synthesis and purified with high-performance liquid chromatography (HPLC) (11). DOTA-TNYL-RAW was prepared by reaction of TNYL-RAW with DOTA-N-hydroxysuccinate, followed by HPLC purification. DOTA-TNYL-RAW was eluted as a single peak, and its mass (2,092.0554 for [M+H]^+^) was confirmed with mass spectroscopy. DOTA-TNYL-RAW (~5 nmol) was incubated with 74–148 MBq (2–4 mCi) ^64^CuCl_2_ in sodium acetate buffer (pH 5.2) for 1 h at 70°C. ^64^Cu-DOTA-TNYL-RAW exhibited a radiochemical purity of >95% as determined with HPLC. The specific activity of ^64^Cu-DOTA-TNYL-RAW was 7.4–14.8 MBq/nmol (0.2–0.4 mCi/nmol) at the end of synthesis. ^nat^Cu-DOTA-TNYL-RAW was prepared similarly. ^64^Cu-DOTA-TNYL-RAW was stable in medium containing 10% fetal bovine serum for up to 24 h at 37°C, whereas only 70% of ^64^Cu-DOTA-TNYL-RAW was intact in mouse serum after 2 h at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20TNYL-RAW%20in+vitro)]

Xiong et al. (11) performed binding experiments with TNYL-RAW, DOTA-TNYL-RAW, and ^nat^Cu-DOTA-TNYL-RAW using a Biacore sensor chip immobilized with EphB4-Fc. The dissociation constant (K_d_) values of TNYL-RAW, DOTA-TNYL-RAW, and ^nat^Cu-DOTA-TNYL-RAW were calculated to be 3.06 nM, 23.3 nM, and 1.98 nM, respectively. No binding to EphB4 was detected with a scrambled TNYL-RAW peptide. In vitro binding of FITC-TNYL-RAW to PC-3M human prostate cancer cells (EphB4-expressing), CT26 human colon cancer cells (EphB4-expressing), and A549 human lung adenocarcinoma cells (EphB4-negative) was determined with fluorescence microscopy. PC-3M and CT26 cells, but not A549 cells, were readily stained with FITC-TNYL-RAW. The binding of FITC-TNYL-RAW to PC-3M and CT26 cells was almost completely blocked by co-incubation with 100-fold excess TNYL-RAW. No binding of FITC-scrambled TNYL-RAW to PC-3M and CT26 cells was observed. ^64^Cu-DOTA-TNYL-RAW exhibited increased cellular uptake with time in PC-3M and CT26 cells but not in A549 cells. Incubation with 100-fold excess of TNYL-RAW almost completely inhibited the radioactivity in PC-3M cells at 30, 60, and 120 min of incubation.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20TNYL-RAW+rodentia)]

Xiong et al. (11) performed PET imaging and ex vivo biodistribution studies of ^64^Cu-DOTA-TNYL-RAW in nude mice (n = 4/group) bearing CT26, PC-3M, and A549 tumors at 1, 4, and 24 h after intravenous injection. Tumors were clearly visualized at 4 h for CT26 tumors and at 4 h and 24 h for PC-3M tumors. PET imaging estimated tumor accumulation values of 1.3% injected dose/gram (ID/g), 2.6% ID/g, and <0.5% ID/g at 1, 4, and 24 h after injection in CT26 tumors, respectively. Tumor accumulation values in PC-3M tumors were 1.4% ID/g, 3.2% ID/g, and 3.6% ID/g at 1, 4, and 24 h after injection, respectively. A549 tumor accumulation values were low, with 1.7% ID/g, 1.5% ID/g, and 1.2% ID/g at 1, 4, and 24 h after injection, respectively. Co-injection of excess TNYL-RAW reduced the radioactivity accumulation by 77% and 81% in CT26 (4 h) and PC-3M (24 h) tumors, respectively.

Ex vivo tumor accumulation was 0.84% ID/g for PC-3M tumors and 0.44% ID/g for A549 tumors at 24 h after injection. Accumulation in the liver, spleen, and kidneys was higher than in the tumors. Co-injection of excess TNYL-RAW inhibited tumor/muscle ratios (~10) for CT26 tumors by 57% and PC-3M tumors by 48% at 4 h and 24 h after injection, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20TNYL-RAW+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20TNYL-RAW+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20TNYL-RAW+human)]

No publication is currently available.

## References

1 Dodelet V.C., Pasquale E.B. (2000). Eph receptors and ephrin ligands: embryogenesis to tumorigenesis. Oncogene.
2 Pasquale E.B. (1997). The Eph family of receptors. Curr Opin Cell Biol.
3 Adams R.H., Klein R. (2000). Eph receptors and ephrin ligands. essential mediators of vascular development. Trends Cardiovasc Med.
4 Cheng N., Brantley D.M., Chen J. (2002). The ephrins and Eph receptors in angiogenesis. Cytokine Growth Factor Rev.
5 Murai K.K., Pasquale E.B. (2011). Eph receptors and ephrins in neuron-astrocyte communication at synapses. Glia.
6 Noren N.K., Lu M., Freeman A.L., Koolpe M., Pasquale E.B. (2004). Interplay between EphB4 on tumor cells and vascular ephrin-B2 regulates tumor growth. Proc Natl Acad Sci U S A.
7 Pasquale E.B. (2010). Eph receptors and ephrins in cancer: bidirectional signalling and beyond. Nat Rev Cancer.
8 Pfaff D., Heroult M., Riedel M., Reiss Y., Kirmse R., Ludwig T., Korff T., Hecker M., Augustin H.G. (2008). Involvement of endothelial ephrin-B2 in adhesion and transmigration of EphB-receptor-expressing monocytes. J Cell Sci.
9 Noren N.K., Pasquale E.B. (2007). Paradoxes of the EphB4 receptor in cancer. Cancer Res.
10 Koolpe M., Burgess R., Dail M., Pasquale E.B. (2005). EphB receptor-binding peptides identified by phage display enable design of an antagonist with ephrin-like affinity. J Biol Chem.
11 Xiong C., Huang M., Zhang R., Song S., Lu W., Flores L., Gelovani J., Li C. (2011). In vivo small-animal PET/CT of EphB4 receptors using 64Cu-labeled peptide. J Nucl Med.